# Pyridine-tetra-acetate-gadolinium(III) (PTA-Gd) conjugated to 17β-estradiol (EPTA-Gd) or tamoxifen (TPTA-Gd)

Chemical name: | Pyridine-tetra-acetate-gadolinium(III) (PTA-Gd) conjugated to 17β-estradiol (EPTA-Gd) or tamoxifen (TPTA-Gd)
Abbreviated name: | EPTA-Gd; TPTA-Gd
Synonym:
Agent Category: | Compounds
Target: | Estrogen receptor α (ER)
Target Category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Estrogen%20receptor%20alpha&cmd=DetailsSearch)]

The luminal-A subtype of breast cancer (the other three subtypes are basal-like, epidermal growth factor receptor 2-positive, and luminal-B (1)) is characterized by overexpression of the estrogen receptor α (ERα) and has been reviewed by Geyer et al. (2). The biological activity and the mode of action of this receptor in the nucleus of a cell have been described by Nilsson et al. (3). In addition, ERα is known to promote cell proliferation that leads to the development of cancerous tumors in the breast (4). Therefore, the ERα is a major biomarker for the detection of ERα-positive (ER+) breast cancer, and the level of its expression in this malignancy is used to predict the response and the prognosis of anti-hormonal therapy for a patient (5). Currently, immunohistochemistry and ELISA are the most common methods used to determine the levels of ER in cancerous breast tissue, but these procedures require the use of invasive techniques to obtain biopsy samples from the primary tumor, and results generated from these tests show analytical variability due to a lack of standardized methods (6). Investigators have successfully used 16α-[^18^F]-fluoro-17β-estradiol ([^18^F]-FES) with positron emission tomography (PET) for the diagnostic imaging of ER+ breast cancer, but this technique may not visualize minute metastasized lesions, and the uptake of [^18^F]-FES by the tumors has been shown to be blocked by estrogen analogs such as tamoxifen (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=407a372d-4448-4d53-afd4-eb0e74bbc336), a drug often used to treat breast cancer (6). Investigators have also used radiolabeled ER ligands with single-photon emission tomography (SPECT) to visualize this receptor in the breast tissue (7); however, no PET or SPECT agents have been approved by the United States Food and Drug Administration for the detection of ER+ tumors (8).

Recently, a magnetic resonance imaging (MRI) probe that targets the ER, pyridine-tetra-acetate-gadolinium(III) (PTA-Gd) conjugated to 17β-estradiol (EPTA-Gd), was synthesized and evaluated for the visualization of ER+ tumors in a mouse model of human breast cancer (8). In the same study, tamoxifen conjugated to PTA-Gd (TPTA-Gd) was also investigated for the imaging of these tumors.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Estradiol%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Estrogen receptor gene information (http://www.ncbi.nlm.nih.gov/gene/2099); Gene ID: 2099 (NCBI)

Estrogen receptor in Online Mendelian Inheritance in Man database (OMIM (http://omim.org/entry/133430))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Estrogen+receptor) related to estrogen receptor

Estrogen receptor imaging clinical trials (http://clinicaltrials.gov/ct2/results?term=Estrogen+receptor+imaging)

Estrogen replacement therapy (http://www.webmd.com/menopause/estrogen-replacement-therapy-ert-16198)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20synthesis&cmd=DetailsSearch)]

The synthesis of PTA-Gd, TPTA-Gd, and EPTA-Gd has been described by Pais et al. (8). The chemical yields of TPTA-Gd and EPTA-Gd were reported to be 8-% and 86%, respectively. The T_1_ relaxation rates (r_1_) of TPTA-Gd, and EPTA-Gd measured at 9.4T were reported to be 4.7 ± 0.1 L/mmol/s and 6.8 ± 0.05 L/mmol/s, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20in%20vitro&cmd=DetailsSearch)]

In an ERα competitive binding assay with ^3^H-labeled 17β-estradiol as the ER binding ligand, the K_i_ of EPTA-Gd and TPTA-Gd were determined to be 0.97 ± 0.07 μmol/L and 0.13 ± 0.006 μmol/L, respectively (8). The proton r_1_ relaxivities of PTA-Gd (control), EPTA-Gd, and TPTA-Gd were measured in solution at 9.4 T and reported to be 3.0 ± 0.1(L/mmol)/s, 6.8 ± 0.7(L/mmol)/s, and 4.7 ± 0.1 (L/mmol)/s, respectively.

MDA-MB-231 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-26&Template=cellBiology) cells (origin: human breast adenocarcinoma) transfected with a tetracycline-inducible ER gene (ER+ cells) were reported to have ER levels between 11,000 and 14,000 fmol/mg protein (8). Wild-type MDA-MB-231 cells (ER− cells) served as controls.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20in%20vivo%20studies&cmd=DetailsSearch)]

Mice bearing tumors in the mammary fat pad (originating from ER+ and ER− cells, respectively) of the animals were used for the in vivo work described in this section (8). Both types of tumors grew at the same rate in the animals, and ER was induced in the ER+ tumors by exposing the animals to doxycycline as described elsewhere (8). Induction of ER in the two tumor types was confirmed with immunostaining in the tumor tissue. Only the ER+ lesions showed strong ER staining in the nucleus, whereas very low staining was observed in the ER− tumor cell organelle.

The biodistribution of PTA-Gd, EPTA-Gd, and TPTA-Gd was studied in severe combined immune deficient mice (n = 5–6 animals/group for each compound) by injecting either 0.1 mmol/kg EPTA-Gd or 0.075 mmol/kg PTA-Gd and TPTA-Gd, respectively, through the tail vein of each rodent in a group (8). Approximately 50 min postinjection (p.i.), organs of interest were harvested from the animals to extract and measure with inductively coupled plasma-mass spectroscopy the amount of Gd(III) accumulated in the tissues. Results obtained from this study were presented as μg Gd/gram tissue (μg Gd/g). At 50 min p.i., PTA-Gd had cleared from most tissues and was present mainly in the kidneys (~40 μg Gd/g); EPTA-Gd accumulated primarily in the liver (~100 μg Gd/g), and TPTA-Gd was detected in the liver (~80 μg Gd/g), kidneys (~70 μg Gd/g), uterus (~30 μg Gd/g), and muscle (~20 μg Gd/g). This indicated that each of the contrast agents had a distinct biodistribution profile. Low amounts of the three contrast agents (less than ~5 μg Gd/g) were present in the brain. In addition, the probes showed a biphasic clearance from blood circulation, which is an initial rapid decrease in concentration followed by a gradual loss.

For in vivo MRI studies, mice bearing ER+ and ER− tumors were injected with 0.075 mmol/kg EPTA-Gd (n = 4–5 animals) and 0.15 mmol/kg TPTA-Gd or PTA-Gd (n = 4 animals/compound), respectively (8). The instrument settings and acquisition of MR images from the animals (under anesthesia) were described by Pais et al. (8). With EPTA-Gd, a significantly higher contrast (measured as percentage (%) enhancement over whole tumor volume) was observed in the ER+ tumors (46.1 ± 21.4%; P = 0.05) compared with the ER− lesions (28.3 ± 2.6%). Both TPTA-Gd and PTA-Gd showed a similar increase in contrast (P > 0.2) in the two types of tumors, indicating that these agents had no specific interaction or binding with the ER. At 40–45 p.i., EPTA-Gd had a contrast of 39.7 ± 17.7% in the ER+ tumors compared with 13.7 ± 3.3% in the muscles (P < 0.005). At the same time point, TPTA-Gd showed a significantly higher contrast (P < 0.01) in the muscles (28.5 ± 6.4%) compared with the ER+ tumors (12.2 ± 1.3%), indicating that this probe bound an unknown component(s) in the muscle.

For a blocking study, animals bearing ER+ and ER− tumors were given an intraperitoneal injection of tamoxifen (final dose, 0.07 mmol/kg; n = 3 mice) or 4-hydroxytamoxifen (final dose, 0.1 mmol/kg; n = 1 mouse) 1 h before the administration of EPTA-Gd through the tail vein (8). The MR images were acquired from the animals as described above. Images acquired at 20–25 min p.i. showed no significant difference in the contrast (P = 0.54) between the ER+ (38.4 ± 16.6%) and the ER− (29.1 ± 12.2%) tumors, and a similar pattern was evident at 40–45 min p.i. (contrast levels for the ER+ and the ER− tumors at this time point were 28.7 ± 7.1% and 29.4 ± 9.5%, respectively; P = 0.93). In addition, the contrast of the ER+ tumors in the anti-estrogen pretreated animals was not significantly different from that of the muscles (31.2 ± 7.0%, P = 0.36 at 20–25 min p.i., and 25.6 ± 6.5%, P =0.43 at 40–55 min p.i.). This study indicated that EPTA-Gd had a binding specificity for the ER.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EPTA-Gd%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported by National Institutes of Health grant CA42238.

## References

1 Tran B., Bedard P.L. (2011). Luminal-B breast cancer and novel therapeutic targets. Breast Cancer Res.
2 Geyer F.C., Rodrigues D.N., Weigelt B., Reis-Filho J.S. (2012). Molecular classification of estrogen receptor-positive/luminal breast cancers. Adv Anat Pathol.
3 Nilsson S., Koehler K.F., Gustafsson J.A. (2011). Development of subtype-selective oestrogen receptor-based therapeutics. Nat Rev Drug Discov.
4 Sekar T.V., Dhanabalan A., Paulmurugan R. (2011). Imaging cellular receptors in breast cancers: an overview. Curr Pharm Biotechnol.
5 Li M.J., Greenblatt H.M., Dym O., Albeck S., Pais A., Gunanathan C., Milstein D., Degani H., Sussman J.L. (2011). Structure of estradiol metal chelate and estrogen receptor complex: the basis for designing a new class of selective estrogen receptor modulators. J Med Chem.
6 van Kruchten, M., A.W. Glaudemans, E.F. de Vries, R.G. Beets-Tan, C.P. Schroder, R.A. Dierckx, E.G. de Vries, and G.A. Hospers, PET Imaging of Estrogen Receptors as a Diagnostic Tool for Breast Cancer Patients Presenting with a Clinical Dilemma. J Nucl Med, 2012
7 Yurt A., Muftuler F.Z., Unak P., Yolcular S., Acar C., Enginar H. (2009). Synthesis of a novel antiestrogen radioligand (99mTc-TOR-DTPA). Cancer Biother Radiopharm.
8 Pais A., Gunanathan C., Margalit R., Eti B.I., Yosepovich A., Milstein D., Degani H. (2011). In vivo magnetic resonance imaging of the estrogen receptor in an orthotopic model of human breast cancer. Cancer Res.